# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-dihistidine-norleucine peptide analog

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-dihistidine-norleucine peptide analog
Abbreviated name: | ^111^In-DOTA-H2-Nle
Synonym: | Radiolabeled minigastrin
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2, CCK-B) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about.the CCK-2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29)]

^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-dihistidine-norleucine peptide (^111^In-DOTA-H2-Nle) is a radiolabeled gastrin analog that can be used for single-photon emission computed tomography (SPECT) imaging of tumors that express the gastrin/cholecystokinin-2 (CCK-2) receptor (1). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The gastrointestinal peptides gastrin and CCK have various regulatory functions in the brain and gastrointestinal tract (2). Gastrin and CCK have the same COOH-terminal pentapeptide amide sequence, which is the biologically active site (3). Human gastrin is a peptide composed of 34 amino acids and also exists in several C-terminal–truncated forms (1). These C-terminal–truncated forms include minigastrin, which is a 13-residue peptide with the sequence of LEEEEEAYGWMDF-NH_2_. CCKs exist in a variety of biologically active molecular forms that are derived from a precursor molecule comprising 115 amino acids (4). These forms range from 4 to 58 amino acids in length and include sulphated and unsulphated CCK-8, which has the structure DYMGWMDF-NH_2_. They bind to and act through transmembrane G-protein–coupled receptors (5). Two different CCK receptor subtypes have been identified in normal tissues. CCK-1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK-2 (CCK-B, brain) receptors have high affinity for gastrin (4). They also differ in terms of molecular structure, distribution, and affinity for CCK. These receptors have also been found to be expressed or overexpressed in a multitude of tumor types (5). CCK-2 receptors have been found most frequently in medullary thyroid carcinomas, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (2). CCK-1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastomas.

Reubi et al. (6) designed a series of radiolabeled CCK-8 peptides that showed high specificity for potential in vivo imaging of tumors expressing CCK-2 receptors. de Jong et al. (7) developed an ^111^In-labeled unsulphated CCK8 analog that used 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) as a bifunctional chelating agent. The radioligand showed high specific internalization rates in receptor-positive rat pancreatic AR42J tumor cells. von Guggenberg et al. (8) reported the synthesis of ^99m^Tc-hydrazinonicotinic acid (HYNIC)-minigastrin complexes and high tumor uptake in nude mice bearing AR42J tumors. Nock et al. (9) prepared ^99m^Tc-labeled minigastrin analogs and found that they displayed high specific localization in nude mice bearing AR42J tumors. Mather et al. (1) synthesized a library of different peptide sequences based on the C-terminal sequences of CCK-8 or minigastrin. These peptides were labeled with ^111^In by DOTA or diethylene triamine pentaacetic acid (DTPA) conjugation. The dihistidine analog ^111^In-DOTA-H2-Nle was evaluated to study the effect of substituting a norleucine (Nle) residue for the methionine (Met) residue near the C-terminus. The study appeared to show that this substitution could result in a reduction in tumor uptake of the radiopeptide analog.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20synthesis)]

The peptide sequence HHEAYGWMDF-amide was obtained by solid-phase peptide synthesis under standard conditions from commercial sources (1). The N-terminus was capped with a DOTA chelating group to produce DOTA-H2-Nle. The identity and purity were confirmed by matrix-assisted laser desorption/ionization mass spectroscopy and reverse-phase high-performance liquid chromatography. Radiolabeling was performed by mixing ^111^In-chloride in ammonium acetate and 0.04 M monothioglycerol (MTG), an antioxidant, with DOTA-H2-Nle in 0.01 M phosphate-buffered saline (pH 7.2). The mixture was heated at 98ºC for 15 min, and 0.1 M ethylenediamine tetraacetic acid (EDTA) was then added to quench the reaction. The labeling yield was >90%. The radiochemical purity and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20in%20vitro)]

An in vitro receptor affinity assay was performed with AGS human gastric tumor cells transfected with the CCK-2 receptor (AGS-CCK2R) and ^125^I-G17 as the radioligand. The inhibition constant (K_i_) and half of the maximum binding fraction (EC_50_) of unlabeled DOTA-H2-Nle were 16.7 nM and 11.3 nM, respectively. In comparison, the K_i_ and EC_50_ of DOTA-H2-Met were 5.7 nM and 3.9 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20rodentia)]

Biodistribution studies of ^111^In-DOTA-H2-Nle were performed in nude mice bearing rat pancreatic AR42J tumors or rat pancreatic CA20948 tumors (1). Both AR42J and CA20948 tumors expressed gastrin receptors. Each mouse received 0.2 μg of ^111^In-DOTA-H2-Nle by i.v. injection. The tumor radioactivity levels at 4 h (n = 3–4), represented as the percentage of injected dose per gram (% ID/g), were 0.73 ± 0.14 and 0.53 ± 0.08 for AR42J and CA20948, respectively. The blood radioactivity levels (% ID/g) at 4 h were 0.03 ± 0.00 and 0.03 ± 0.00 for AR42J and CA20948 tumors, respectively. The kidney radioactivity levels (% ID/g) at 4 h were 2.40 ± 2.13 and 1.73 ± 0.31 for AR42J and CA20948 tumors, respectively. No blocking study was performed. In comparison, the tumor radioactivity levels (% ID/g) of ^111^In-DOTA-H2-Met at 4 h were 0.87 ± 0.21 and 0.59 ± 0.10 for AR42J and CA20948 tumors, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20human)]

No publication is currently available.

## References

1 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
2 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
3 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 Reubi J.C., Waser B. (1996). Unexpected high incidence of cholecystokinin-B/gastrin receptors in human medullary thyroid carcinomas. Int J Cancer.
7 de Jong M., Bakker W.H., Bernard B.F., Valkema R., Kwekkeboom D.J., Reubi J.C., Srinivasan A., Schmidt M., Krenning E.P. (1999). Preclinical and initial clinical evaluation of 111In-labeled nonsulfated CCK8 analog: a peptide for CCK-B receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
8 von Guggenberg E., Behe M., Behr T.M., Saurer M., Seppi T., Decristoforo C. (2004). 99mTc-labeling and in vitro and in vivo evaluation of HYNIC- and (Nalpha-His)acetic acid-modified [D-Glu1]-minigastrin. Bioconjug Chem.
9 Nock B.A., Maina T., Behe M., Nikolopoulou A., Gotthardt M., Schmitt J.S., Behr T.M., Macke H.R. (2005). CCK-2/gastrin receptor-targeted tumor imaging with (99m)Tc-labeled minigastrin analogs. J Nucl Med.